# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-polyethylene glycol-single-chain Cys-tagged vascular endothelial growth factor-121

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-polyethylene glycol-single-chain Cys-tagged vascular endothelial growth factor-121
Abbreviated name: | ^64^Cu-DOTA-PEG-scVEGF
Synonym:
Agent Category: | Polypeptide
Target: | VEGF receptors
Target Category: | Receptor-ligand binding
Method of detection: | PET
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71051581), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001025368.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=7422) for more information about VEGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF)]

Vascular endothelial growth factor (VEGF) consists of at least six isoforms with various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (1). VEGF_121_, VEGF_165_, and VEGF_189_ are the forms secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like the other VEGF species (2). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors on endothelial cells (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4). Several types of non-endothelial cells such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells also express VEGF receptors (1).

VEGF receptors were found to be overexpressed in various tumor cells and tumor-associated endothelial cells (3). Inhibition of VEGF receptor function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (4, 5). Radiolabeled VEGF has been developed as a tracer for imaging solid tumors and angiogenesis in humans (6-8). Cys-tag, a fusion tag comprising 15 amino acids, was developed for site-specific conjugation via the free sulfhydryl group of Cys. Backer et al. (9) prepared a Cys-tagged vector of VEGF_121_ by cloning two single-chain fragments (3–112 amino acids long) of VEGF_121_ joining head-to-tail to express as scVEGF, which can be labeled as (^64^Cu-DOTA-scVEGF), ^99m^Tc-hydrazinonicotinic acid (HYNIC)-scVEGF (^99m^Tc-HYNIC-scVEGF), and Cy5.5-scVEGF for imaging VEGFR expression to study tumor angiogenesis (10). ^64^Cu-DOTA-PEG-scVEGF is being developed for positron emission tomography (PET) imaging of VEGFR-2 in tumor vasculature.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+synthesis)]

Backer et al. (9) prepared a Cys-tagged vector of VEGF_121_ by cloning two single-chain fragments (amino acid sequence 3–112) of VEGF_121_ joining head-to-tail to express as scVEGF in Escherichia coli for mammalian cell production. ^64^Cu labeling of scVEGF was performed through DOTA chelation. DOTA was activated by a five-fold molar excess of N-hydroxysuccinimide-polyethylene glycol (PEG)-maleimide (pH 8) for 60 min (10). A mixture of scVEGF and the activated DOTA in a molar ratio of 1:10 was incubated for 60 min. The DOTA-PEG-scVEGF conjugate was purified with high-performance liquid chromatography. The number of DOTA molecules per protein was ~1. For radiolabeling, 20 μg of scVEGF was added to 18.5 MBq (0.5 mCi) of ^64^Cu diluted in 0.1 M sodium acetate buffer (pH 5.5). The reaction mixture was incubated at 55ºC for 1 h. ^64^Cu-DOTA-PEG-scVEGF was purified with column chromatography with a radiolabeling yield of 40%. ^64^Cu-DOTA-PEG-inVEGF, used as an inactive control, was prepared by conjugation of 7–8 biotins to ^64^Cu-DOTA-PEG-scVEGF. The extensive biotinylation of ^64^Cu-DOTA-PEG-scVEGF probably destroys the binding capacity of scVEGF.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+and+in+vitro)]

In vitro competition binding studies were performed in 293/KDR cells expressing cloned human VEGFR-2 in competition with the chimeric toxin SLT-VEGF for binding to VEGFR-2 (10). ^64^Cu-DOTA-PEG-scVEGF, DOTA-PEG-scVEGF, HYNIC-scVEGF, and Cy5.5-scVEGF inhibited the binding of SLT-VEGF to VEGFR-2. Saturation binding was performed with ^64^Cu-DOTA-PEG-scVEGF to provide a dissociation constant of 2.8 nM and a maximum binding of 1.3 × 10^6^ binding sites per cell. DOTA-PEG-scVEGF, HYNIC-scVEGF, and Cy5.5-scVEGF stimulated tyrosine phosphorylation of VEGFR-2 in 293/KDR cells in a manner similar to VEGF. ^64^Cu-DOTA-PEG-scVEGF was >95% intact after incubation in mouse plasma or radiolabeling buffer at 37ºC for 5 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+rodentia)]

Backer et al. (10) performed biodistribution studies of ^64^Cu-DOTA-PEG-scVEGF in mice bearing 4T1 murine breast tumors expressing VEGFR-2. The tumor accumulated ~3% injected dose per gram (% ID/g), whereas the muscle accumulated ~0.5% ID/g. The organs with the highest accumulation of ^64^Cu-DOTA-PEG-scVEGF were the kidneys (~60% ID/g), liver (~8% ID/g), and lung (~5% ID/g) at 2 h after injection. PET imaging studies were performed at 1, 3, and 9 h after injection of ^64^Cu-DOTA-PEG-scVEGF or ^64^Cu-DOTA-PEG-inVEGF. ^64^Cu-DOTA-PEG-scVEGF revealed higher and more heterogeneous focal accumulation than ^64^Cu-DOTA-PEG-inVEGF. Pre-incubation of ^64^Cu-DOTA-PEG-scVEGF with KDR-Fc (VEGFR-2) before injection greatly reduced the tumor accumulation.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+human)]

No publication is currently available.

## NIH Support

R21 EB001946, R43 CA113080, P50 CA114747, CA064436

## References

1 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
2 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
3 Soria J.C., Fayette J., Armand J.P. (2004). Molecular targeting: targeting angiogenesis in solid tumors. Ann Oncol.
4 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
5 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
6 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
7 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
8 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
9 Backer M.V., Patel V., Jehning B.T., Claffey K.P., Backer J.M. (2006). Surface immobilization of active vascular endothelial growth factor via a cysteine-containing tag. Biomaterials.
10 Backer M.V., Levashova Z., Patel V., Jehning B.T., Claffey K., Blankenberg F.G., Backer J.M. (2007). Molecular imaging of VEGF receptors in angiogenic vasculature with single-chain VEGF-based probes. Nat Med.